# Cy5.5-c(Lys-Ala-His-Trp-Gly-Phe-Thr-Leu-Asp)NH_2_

Chemical name: | Cy5.5-c(Lys-Ala-His-Trp-Gly-Phe-Thr-Leu-Asp)NH_2_
Abbreviated name: | Cy5.5-C6
Synonym: | Cy5.5-c(KAHWGFTLD)NH_2_
Agent category: | Peptide
Target: | Gelatinases (MMP-2 and MMP-9)
Target category: | Enzyme
Method of detection: | Optical, near-infrared fluorescence (NIR)
Source of signal: | Cy5.5
Activation: | No
Studies: | - In vitro; - Rodents | Click on MMP-2 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=116856) and MMP-9 (http://www.ncbi.nlm.nih.gov/entrez/viewer.fcgi?db=protein&id=10443048) for protein information.

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6)]

Optical fluorescence imaging is increasingly being used to monitor biological functions of specific targets in small animals (1-3). However, the intrinsic fluorescence of biomolecules poses a problem when fluorophores that absorb visible light (350–700 nm) are used. Near-infrared (NIR) fluorescence (700–1,000 nm) detection avoids the natural background fluorescence interference of biomolecules, providing a high contrast between target and background tissues in small animals. NIR fluorophores have a wider dynamic range and minimal background fluorescence as a result of reduced scattering compared with visible fluorescence detection. NIR fluorophores also have high sensitivity, attributable to low background fluorescence, and high extinction coefficients, which provide high quantum yields. The NIR region is also compatible with solid-state optical components, such as diode lasers and silicon detectors. NIR fluorescence imaging is a non-invasive alternative to radionuclide imaging in small animals.

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (4). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (5). Invasive tumor cells adhere to the ECM, which provides a matrix environment for permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (6).

Several families of proteases are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (7-10). The gelatinase family is a subgroup of MMPs consisting of gelatinase A (MMP-2) and gelatinase B (MMP-9) (11). Gelatinase expression in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages, is highly regulated. Elevated levels of gelatinases have been found in tumors associated with a poor prognosis for cancer patients (12). A cyclic peptide, c(CTTHWGFTLC)NH_2_ (C1), was identified by phage screening to be potent inhibitor of MMP-2 and MMP-9 (13); however, C1 is readily degraded in vivo. A synthetic peptide, c(KAHWGFTLD)NH_2_ (C6), was linked with a Cy5.5 NIR dye molecule via the α-NH_2_ of Lys to form Cy5.5-C6 for in vivo imaging of MMP-2/-9 activity (14). Cy5.5-C6 is being developed for NIR fluorescence imaging of MMP-2/-9 proteolytic activity in tumors.

### Related Resource Links:

- Chapters in MICAD (http://www.ncbi.nlm.nih.gov/sites/entrez?db=Books&cmd=Search&term=MMP+AND+micad%5bbook%5d&doptcmdl=TOCView&log%24=booksrch&bname=micad)
- Gene information in NCBI (Gelatinases (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=gene&Cmd=DetailsSearch&Term=Gelatinases)).
- Articles in OMIM (http://www.ncbi.nlm.nih.gov/omim/?term=Gelatinases)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6+synthesis)]

C6 was synthesized using Fmoc solid-phase chemistry (14). Cy5.5-Monofunctional N-hydroxysuccinimide ester (1.3 µmol) was used to conjugate the α-amino group of Lys (1 µmol) to form Cy5.5-C6, which was purified with high-performance liquid chromatography (HPLC). The reaction was carried out for 18 h at room temperature. Cy5.5-C6 was identified with analytical HPLC and mass spectrometry. Cy5.5-C1 and Cy5.5-C7 (scrambled peptide) were also prepared as controls. Cy5.5 has an absorbance maximum at 675 nm and an emission maximum at 694 nm with a high extinction coefficient of 250,000 M^-1^cm^-1^. Cy5.5-C6 exhibited a fluorescence emission spectrum similar to that of Cy5.5. C6 was stable in medium containing bovine serum for 3 h at room temperature, whereas C1 was completely degraded by 3 h.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6%20and+in+vitro)]

Cy5.5 interferes with the MMP-2 enzyme fluorescence assay. Therefore, Cy5.5-C1 and Cy5.5-C6 (10–200 μM) was evaluated in a different assay showing inhibition of degradation of β-casein (1 μg) by activated MMP-2 (100 ng). Wang et al. (14) showed that C1 and C6 inhibited MMP-2 activity with 50% inhibition concentration (IC_50_) values of 30.3 and 7.6 µM, respectively. Fluorescence confocal microscopy showed that Cy5.5-C6 (10 μM) was readily taken up by MMP-2–positive human glioma U87 and prostate PC3 tumor cells in culture but not by MMP-2–negative A549 human lung tumor cells. Cy5.5-C1 (10 μM) was taken up to a lesser extent by U87 tumor cells. The uptake of Cy5.5-C6 by U87 tumor cells was inhibited by the MMP inhibitor doxycycline (100 μM).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6+rodentia)]

Wang et al. (14) performed fluorescence imaging studies of 15 nmol Cy5.5-C1, Cy5.5-C6, and Cy5.5-C7 in mice bearing PC3 tumors. Images were obtained at 48 h after injection. Accumulation of Cy5.5-C6 was clearly visualized in the tumors, whereas Cy5.5-C1 and Cy5.5-C7 exhibited little accumulation in the tumors. In another experiment, Cy5.5-C6 was administered to mice bearing orthotopical U87 gliomas. Accumulation of Cy5.5-C6 was clearly visualized in the tumors. Zymography experiments showed that MMP-2 expression in the tumor tissue. Ex vivo optical imaging showed tumor/background ratio of 3.30 ± 0.64. No blocking and MMP inhibition experiments were performed.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6+(dog+or+pig+or+sheep+or+rabbit))]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6+(primate+not+human))]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=Cy5.5-C6+human)]

No publication is currently available.

## NIH Support

R01 EB000174, U54 CA90810

## References

1 Achilefu S. (2004). Lighting up tumors with receptor-specific optical molecular probes. Technol Cancer Res Treat.
2 Ntziachristos V., Bremer C., Weissleder R. (2003). Fluorescence imaging with near-infrared light: new technological advances that enable in vivo molecular imaging. Eur Radiol.
3 Becker A., Hessenius C., Licha K., Ebert B., Sukowski U., Semmler W., Wiedenmann B., Grotzinger C. (2001). Receptor-targeted optical imaging of tumors with near-infrared fluorescent ligands. Nat Biotechnol.
4 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
5 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
6 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
7 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
8 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
9 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
10 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
11 Nelson A.R., Fingleton B., Rothenberg M.L., Matrisian L.M. (2000). Matrix metalloproteinases: biologic activity and clinical implications. J Clin Oncol.
12 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
13 Koivunen E., Arap W., Valtanen H., Rainisalo A., Medina O.P., Heikkila P., Kantor C., Gahmberg C.G., Salo T., Konttinen Y.T., Sorsa T., Ruoslahti E., Pasqualini R. (1999). Tumor targeting with a selective gelatinase inhibitor. Nat Biotechnol.
14 Wang W., Shao R., Wu Q., Ke S., McMurray J., Lang F.F., Charnsangavej C., Gelovani J.G., Li C. (2009). Targeting gelatinases with a near-infrared fluorescent cyclic His-Try-Gly-Phe peptide. Mol Imaging Biol.